# [^64^Cu](1-N-(4-aminobenzyl)-3,6,10,13,16,19-hexaazabicyclo[6.6.6]-eicosane-1,8-diamine)-anti-GD2 monoclonal antibody

Chemical name: | [^64^Cu](1-N-(4-aminobenzyl)-3,6,10,13,16,19-hexaazabicyclo[6.6.6]-eicosane-1,8-diamine)-anti-GD2 monoclonal antibody
Abbreviated name: | [^64^Cu]SarAr-anti-GD2 mAb
Synonym: | [^64^Cu]SarAr-mAb
Agent Category: | Monoclonal antibody
Target: | Disialogangliosides
Target Category: | Antibody-ligand binding
Method of detection: | Positron emission tomography (PET)
Source of Signal/Contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

Positron emission tomography (PET) is a common technique used in conjunction with fluorodeoxyglucose labeled with radioactive fluorine ([^18^F]FDG) to investigate metabolism and to detect and evaluate the efficacy of cancer therapy (1, 2). Although a variety of ^18^F-labeled small molecule compounds, their derivatives, and antibodies (including those that were bioengineered) have been developed and evaluated in addition to [^18^F]FDG for PET imaging, the short physical half-life of this isotope (110 min) and the requirement of specialized equipment and personnel for the synthesis of ^18^F derivatives are major limitations for its use in the clinic (3). Investigators have also evaluated the use of radioactive copper (^64^Cu) in an effort to develop PET imaging agents that have a longer half-life (12.7 h); however, biodistribution studies in rats have revealed that transchelation of ^64^Cu to copper binding proteins such as ceruloplasmin and superoxide dismutase in the liver and albumin results in the high background observed with this isotope during imaging (4). In this regard, investigators have been in search of chelating agents that can be used to produce ^64^Cu complexes with an extended stability under in vivo conditions, have good labeling properties, and are easily conjugated to molecules or antibodies with specific targets for PET imaging (5, 6).

Disialogangliosides (GD2) are ubiquitous and abundant surface glycolipid antigens found on tumors of neuroectodermal origin, including melanoma and neuroblastoma tumors. Therefore, these antigens are considered ideal targets for the immunotherapy of these diseases (7, 8). The use of an anti-GD2 monoclonal antibody (mAb) is one of the options available for the treatment of these cancers, and several clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-GD2+monoclonal+antibody) have been approved by the United States Food and Drug Administration for the use of this antibody to treat children and adults. The status of some of the clinical trials being conducted with the anit-GD2 antibody has been reviewed by Modak et al. (7).

Voss et al. developed a novel chelating agent, 1-N-(4-aminobenzyl)-3,6,10,13,16,19-hexaazabicyclo[6.6.6]-eicosane-1,8-diamine (SarAr), that they used to chelate ^64^Cu to an anti-GD2 mAb. The authors evaluated SarAr under in vivo conditions for the imaging of human neuroblastoma and melanoma tumors in athymic mice (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+antiGD2+mAb+synthesis)]

A murine anti-GD2 antibody, 14.G2a, was purchased commercially, and a chimeric derivative of this antibody, ch14.18, was engineered as detailed elsewhere (9). The ch14.18 mAb was used to perform the studies detailed in this chapter. The two antibodies have a similar murine variable region sequence and an identical antigen-binding Fv region, and they were reported to contain distinct constant region sequences (6).

Synthesis of the SarAr chelator was described by Di Bartolo et al. (10). Using 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide (EDC), the SarAr ligand was conjugated through its primary aromatic group to the carboxyl groups of the glutamate and aspartate residues of the 14.G2a and ch14.18 mAbs (6). To achieve this, EDC was added to the mAb in a ratio of 250:1 for SarAr:IgG as described elsewhere using sodium acetate buffer (pH 5.0) at 37°C for 30 min (11). Unbound SarAr was removed from the immunoconjugates with high-performance liquid chromatography (HPLC), and the SarAr-conjugated mAbs were concentrated by use of spin filters for storage at -80°C. Four SarAr molecules were estimated to be bound to each mAb molecule as determined by serial dilution experiments (6).

The SarAr-conjugated antibodies were radiolabeled using [^64^Cu]copper chloride in sodium acetate buffer (pH 5.0) at 37°C for 30 min (6). The investigators reported the same labeling efficiency could also be obtained at 21°C for 10 min. The labeling efficiency was routinely 99% as determined by HPLC and thin-layer chromatography (TLC); the Rf values for TLC were not provided. Specific activity of [^64^Cu]SarAr mAb was reported to be 10 μCi/6.6 nmol (370 kBq/6.6 nmol). An investigation of ^64^Cu-labeled ch14.18 by radioimmunoassay and cell-binding studies showed that the labeled mAb had immunoreactivity similar to the unlabeled mAb (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+SarAr+mAb+in+vitro)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+SarAr+mAb+rodentia)]

Biodistribution studies were performed with athymic nu/nu mice bearing xenograft tumors derived from M21 (human melanoma cells that express high levels of GD2 antigen (12)), IMR-6 (human neuroblastoma cells that express moderate levels of GD2 antigen (13)), or PC-3 cells (human prostate carcinoma cells that are negative for the GD2 antigen) (6). Animals were injected with the ^64^Cu-labeled mAb through the tail vein, and the animals were killed at various time points (n = 4 animals per time point) between 6 and 48 h after administration of the radiotracer. The major organs, including tumors, were then removed and weighed, and incorporated radioactivity was counted. Approximately 15–20% of the radioactivity (injected dose per gram tissue (% ID/g) was determined to be associated with the tumors 24 h after injection of the radiotracer (126.7 ± 0.6% ID/g for the IMR-6 neuroblastoma, 20.5 ± 2.8% ID/g for M21 melanoma cells) (6). Under the same conditions, the GD2-negative xenograft tumors (PC-3) showed a low level of radiotracer incorporation (<5% ID/g). Low levels of radioactivity were observed in the liver of these animals.

PET imaging was performed at 24 and 48 h after the radiotracer injection (6). High accumulation of the label was evident in the GD2-positive tumors with low uptake in the surrounding nontarget tissue, including the liver. These results were in agreement with those obtained from the individual tissue removed from the animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+SarAr+mAb+other+non+primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+SarAr+mAb+non+human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Kumar R., Basu S., Torigian D., Anand V., Zhuang H., Alavi A. (2008). Role of modern imaging techniques for diagnosis of infection in the era of 18F-fluorodeoxyglucose positron emission tomography. Clin Microbiol Rev.
2 Juweid M.E. (2008). 18F-FDG PET as a routine test for posttherapy assessment of Hodgkin's disease and aggressive non-Hodgkin's lymphoma: where is the evidence?. J Nucl Med.
3 Smith S.V. (2004). Molecular imaging with copper-64. J Inorg Biochem.
4 Boswell C.A., Sun X., Niu W., Weisman G.R., Wong E.H., Rheingold A.L., Anderson C.J. (2004). Comparative in vivo stability of copper-64-labeled cross-bridged and conventional tetraazamacrocyclic complexes. J Med Chem.
5 Sprague J.E., Peng Y., Fiamengo A.L., Woodin K.S., Southwick E.A., Weisman G.R., Wong E.H., Golen J.A., Rheingold A.L., Anderson C.J. (2007). Synthesis, characterization and in vivo studies of Cu(II)-64-labeled cross-bridged tetraazamacrocycle-amide complexes as models of peptide conjugate imaging agents. J Med Chem.
6 Voss S.D., Smith S.V., DiBartolo N., McIntosh L.J., Cyr E.M., Bonab A.A., Dearling J.L., Carter E.A., Fischman A.J., Treves S.T., Gillies S.D., Sargeson A.M., Huston J.S., Packard A.B. (2007). Positron emission tomography (PET) imaging of neuroblastoma and melanoma with 64Cu-SarAr immunoconjugates. Proc Natl Acad Sci U S A.
7 Modak S., Cheung N.K. (2007). Disialoganglioside directed immunotherapy of neuroblastoma. Cancer Invest.
8 Riemer A.B., Forster-Waldl E., Bramswig K.H., Pollak A., Zielinski C.C., Pehamberger H., Lode H.N., Scheiner O., Jensen-Jarolim E. (2006). Induction of IgG antibodies against the GD2 carbohydrate tumor antigen by vaccination with peptide mimotopes. Eur J Immunol.
9 Gillies S.D., Lo K.M., Wesolowski J. (1989). High-level expression of chimeric antibodies using adapted cDNA variable region cassettes. J Immunol Methods.
10 Di Bartolo N.M., Sargenson A.M., Donlevy T.M., Smith S.V. (2001). Synthesis of a new cage ligand, SarAr, and its complexation with select transition metal ions for potential use in radioimaging. J Chem Soc Dalton Trans.
11 Di Bartolo N.M., Sargenson A.M., Smith S.V. (2006). New 64Cu PET imaging agents for personalized medicine and drug development using the hexa-aza, SarAr. Organic and Biomolecular Chemistry.
12 Mueller B.M., Reisfeld R.A., Gillies S.D. (1990). Serum half-life and tumor localization of a chimeric antibody deleted of the CH2 domain and directed against the disialoganglioside GD2. Proc Natl Acad Sci U S A.
13 Cheung N.K., Neely J.E., Landmeier B., Nelson D., Miraldi F. (1987). Targeting of ganglioside GD2 monoclonal antibody to neuroblastoma. J Nucl Med.